# ^124^I-Chimeric monoclonal antibody G250

Chemical name: | ^124^I-Chimeric monoclonal antibody G250
Abbreviated name: | ^124^I-cG250
Synonym:
Agent category: | Antibody
Target: | Carbonic anhydrase IX
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=94963095), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=125661057) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=55894&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about human carbonic anhydrase IX.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250)]

In a variety of solid tumors, hypoxia was found to lead to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy. It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized polarographic oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7). This has led to the search for and development of hypoxia-targeted, non-invasive markers of tumor hypoxia.

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic condition, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). [^18^F]Fluoromisonidazole ([^18^F]FMISO) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (7). Carbonic anhydrase (CA) IX is one of the most overexpressed genes in cells under hypoxic conditions (10). It is a transmembrane glycoprotein with CA activity in the extracellular domain, and it is found to be overexpressed in renal cell, cervical, lung, and colorectal tumors. Murine monoclonal antibody G250 against CA IX has been developed for in vitro and in vivo localization of CA IX in cells (11-13). G250 is found to bind to >94% of human clear-cell renal carcinoma. A murine-human chimeric G250 (cG250) has been generated to be less immunogenic in humans (14). ^124^I-cG250 has been evaluated as a PET imaging agent for renal cell carcinoma in mice (15) and patients (16).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Carbonic%20anhydrase%20IX+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Carbonic anhydrase IX (http://www.ncbi.nlm.nih.gov/gene/55894)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=CA%20IX)
- Clinical trials (G250 (http://www.clinicaltrials.gov/ct2/results?term=G250))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250+synthesis)]

The cG250 antibody (~2 nmol) was labeled with 4 MBq (0.108 mCi) ^124^I in the presence of Iodogen (15). ^124^I-cG250 was isolated with size-exclusion column chromatography with a radiolabeling efficiency of 67% and a specific activity of 6.2 MBq/nmol (0.16 mCi/nmol). Thin-layer chromatography revealed >97% of ^124^I was bound to cG250. ^124^I-cG250 exhibited an immunoreactivity of 95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250+in+vitro)]

Lawrentschuk et al. (15) performed binding experiments with ^124^I-cG250 in SK-RC-52 human renal carcinoma cells. The dissociation constant was found to be 2.2 nM with 400,000 antibody molecules per cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250+rodentia)]

Lawrentschuk et al. (15) studied the biodistribution of ^124^I-cG250 in mice (n = 5/group) bearing SK-RC-52 tumors at days 0 (2 h), 2, 3, and 7 after injection. The tracer accumulation in the tumors was 9.6%, 23.5%, 19.4%, and 7.4% injected dose per gram (ID/g), respectively. The liver and kidneys had lower radioactivity levels than the tumors at days 2–7. The radioactivity in the blood decreased from 32.2% ID/g (day 0) to 0.5% ID/g (day 7). The tumor/blood ratios were 5.0 and 31.0 on day 3 and day 7, respectively. The blood clearance pattern exhibited a two-phase model with a half-life of 2.6 h during the distribution phase and a half-life of 40.5 h during the elimination phase. The control antibody ^124^I-huA33 exhibited very low tumor accumulation. No blocking experiment was performed.

PET imaging with ^124^I-cG250 showed localization in the tumors and relatively low activity elsewhere in the mice at 24 h after injection. There was a significant correlation (r^2^ = 0.93, P < 0.0001) between tumor standard uptake values measured with PET and ex vivo measurement (% ID/g). Histoimmunostaining showed CA IX was distributed evenly in the viable tumor cells of the tumor sections.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=124I-cG250+human)]

Divgi et al. (16) performed PET imaging with ^124^I-cG250 in 25 patients with renal masses who were scheduled to undergo surgical resection by laparotomy received a single intravenous infusion of 185 MBq (5 mCi (66 nmol)) ^124^I-cG250 over 20 min in this open-label pilot study. The obtained images were graded as positive (defined as a tumor/healthy kidney ratio >3). Fifteen of 16 clear-cell carcinomas were identified accurately with PET, and all nine non–clear-cell renal masses were negative for the tracer. The sensitivity of ^124^I-cG250 PET for clear-cell kidney carcinoma was 94%; the negative predictive value was 90%, and specificity and positive predictive accuracy were both 100%.

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Loncaster J.A., Harris A.L., Davidson S.E., Logue J.P., Hunter R.D., Wycoff C.C., Pastorek J., Ratcliffe P.J., Stratford I.J., West C.M. (2001). Carbonic anhydrase (CA IX) expression, a potential new intrinsic marker of hypoxia: correlations with tumor oxygen measurements and prognosis in locally advanced carcinoma of the cervix. Cancer Res.
11 Lam J.S., Pantuck A.J., Belldegrun A.S., Figlin R.A. (2005). G250: a carbonic anhydrase IX monoclonal antibody. Curr Oncol Rep.
12 Oosterwijk E., Debruyne F.M. (1995). Radiolabeled monoclonal antibody G250 in renal-cell carcinoma. World J Urol.
13 Grabmaier K., Vissers J.L., De Weijert M.C., Oosterwijk-Wakka J.C., Van Bokhoven A., Brakenhoff R.H., Noessner E., Mulders P.A., Merkx G., Figdor C.G., Adema G.J., Oosterwijk E. (2000). Molecular cloning and immunogenicity of renal cell carcinoma-associated antigen G250. Int J Cancer.
14 Ahlskog J.K., Schliemann C., Marlind J., Qureshi U., Ammar A., Pedley R.B., Neri D. (2009). Human monoclonal antibodies targeting carbonic anhydrase IX for the molecular imaging of hypoxic regions in solid tumours. Br J Cancer.
15 Lawrentschuk, N., F.T. Lee, G. Jones, A. Rigopoulos, A. Mountain, G. O'Keefe, A.T. Papenfuss, D.M. Bolton, I.D. Davis, and A.M. Scott, Investigation of hypoxia and carbonic anhydrase IX expression in a renal cell carcinoma xenograft model with oxygen tension measurements and (124)I-cG250 PET/CT. Urol Oncol, 2009
16 Divgi C.R., Pandit-Taskar N., Jungbluth A.A., Reuter V.E., Gonen M., Ruan S., Pierre C., Nagel A., Pryma D.A., Humm J., Larson S.M., Old L.J., Russo P. (2007). Preoperative characterisation of clear-cell renal carcinoma using iodine-124-labelled antibody chimeric G250 (124I-cG250) and PET in patients with renal masses: a phase I trial. Lancet Oncol.